# (20R)-4,5-α-Epoxy-6-(2-[^18^F])fluoroethoxy)-3-hydroxy-α,17-dimethyl-α-(2-phenyleth-1-yl)-6,14-ethenomorphinan-7-methanol

Chemical name: | (20R)-4,5-α-Epoxy-6-(2-[^18^F]fluoroethoxy)-3-hydroxy-α,17-dimethyl-α-(2-phenyleth-1-yl)-6,14-ethenomorphinan-7-methanol
Abbreviated name: | [^18^F]FE-PEO
Synonym:
Agent category: | Compound
Target: | Opioid receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO)]

Opioids such as morphine are analgesics that are commonly used in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (morphine- and ß-endorphin–preferring) (1). Each type of opioid receptor consists of subtypes of receptors, as suggested by pharmacological studies (2, 3). These receptors exhibit apparent specificity to both the central and the peripheral nervous systems, and their presence is ubiquitous in these systems. The opioid receptors (G-protein–coupled, resulting in decreased adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, and cardiovascular, mental, and endocrine function (2-5). Although µ opioid receptors are the major receptors to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemic injury in the heart and brain via the δ receptors. On the other hand, κ antagonists prevent neurodegeneration.

The µ opioid receptors are localized predominately in the hypothalamus and thalamus, and the δ opioid receptors are localized predominately in the striatum, limbic system, and cerebral cortex (6, 7). The κ opioid receptors (κ_1_ and κ_2_) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, amygdala, and thalamus, with lower levels in the hippocampus, occipital cortex, and cerebellum (8-10). The κ opioid receptors have been implicated in several clinical brain disorders, including drug abuse (11), epilepsy (12), Tourette’s syndrome (13), and Alzheimer’s disease (14).

Diprenorphine is a highly potent and nonselective opioid receptor antagonist with subnanomolar affinity (7). Diprenorphine has been labeled as [6-O-methyl-^11^C]diprenorphine ([^11^C]DPN (http://www.ncbi.nlm.nih.gov/books/NBK23399/)) (15, 16). [^11^C]DPN is being developed as a positron emission tomography (PET) agent for the noninvasive study of opioid receptors in the brain. However, pharmacological studies in humans (17) and rats (18) have demonstrated minimal competition between the high-efficacy agonists and the non-subtype–selective antagonist radioligand [^11^C]DPN, which limits the use of [^11^C]DPN PET to monitor in vivo occupancy (20R). -4,5-α-Epoxy-17-methyl-3-hydroxy-6-methoxy-α,17-dimethyl-α-(2-phenylethyl)-6,14-ethenomorphinan-7-methanol (PEO) has been found to be a highly potent opioid receptor agonist (19). [6-O-methyl-^11^C]PEO ([^11^C]PEO (http://www.ncbi.nlm.nih.gov/books/NBK23280/)) was evaluated for use with PET imaging of opioid receptors in rats, and the agent showed specific accumulation in the striatum, thalamus, and frontal cortex. For ^18^F-labeling, Riss et al. (20) prepared (20R)-4,5-α-epoxy-6-(2-[^18^F]fluoroethoxy)-3-hydroxy-α,17-dimethyl-α-(2-phenyleth-1-yl)-6,14-ethenomorphinan-7-methanol ([^18^F]FE-PEO) for use with PET imaging of opioid receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (opioid receptors (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=Opioid+AND+micad%5Bbook%5D))
- Gene information in NCBI (opioid receptors (http://www.ncbi.nlm.nih.gov/gene?term=opioid%20receptors))
- Articles in Online Mendelian Inheritance in Man (OMIM) (opioid receptors (http://omim.org/search?index=entry&start=1&limit=10&search=opioid++genes&sort=score+desc%2C+prefix_sort+desc))
- Clinical trials (opioid receptors (http://www.clinicaltrials.gov/ct2/results?term=opioid+receptors+))
- Drug information in FDA (opioid receptors (http://google2.fda.gov/search?q=opioid+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO%20and%20synthesis)]

Riss et al. (20) performed synthesis of [^18^F]FE-PEO. The tosyloxyethyl-precursor was subjected to nucleophilic fluorination with K[^18^F]F/Kryptofix2.2.2 for 10 min at 90°C, with a yield of 28 ± 15% and a specific activity of 52–224 GBq/μmol (1.4–6.1 Ci/μmol) after purification with high-performance liquid chromatography. The radiochemical purity of [^18^F]FE-PEO was >97%, and the total synthesis time was ~90 min. [^18^F]FE-PEO was >95% intact in rat blood for 2 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO%20and%20in%20vitro)]

Riss et al. (20) reported in vitro binding assays using membranes of cloned human receptor stably expressed on Chinese hamster ovary (CHO) cells (µ and κ) and on HEK-293 cells (δ). FE-PEO exhibited inhibition constant (K_i_) values of 0.4 ± 0.03 nM, 0.4 ± 0.02 nM, and 1.6 ± 0.2 nM for the µ ([^3^H]DPN), κ ([^3^H]DPN), and δ ([^3^H]naltrindole) opioid receptors, respectively. Therefore, PEO binds to µ and κ subtypes of opioid receptors with slightly higher affinity than the δ subtype.

In vitro [^18^F]FE-PEO autoradiographic imaging studies were performed on rat brain sections (20). [^18^F]FE-PEO bound heterogeneously to the brain sections (n = 24), with high accumulation of radioactivity in the endopiriform nucleus, accumbens, and cingulate cortex. Moderate radioactivity was found in the striatum. Pretreatment of the brain sections (n = 12) with the µ-opioid receptor–selective agonist DAMGO (1,000 nM) reduced radioactivity in the endopiriform nucleus, cingulate cortex, and striatum by 61%, 59%, and 42%, respectively. Pretreatment of the brain sections (n = 12) with the opioid receptor–nonselective antagonist naloxone (10 µM) reduced radioactivity in the endopiriform nucleus, cingulate cortex, and striatum by 63%, 65%, and 66%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO%20and%20rodentia)]

Riss et al. (20) performed dynamic PET imaging studies for 180 min in rats (n = 3) injected with 20 MBq (0.54 mCi) [^18^F]FE-PEO. High distribution volume (V_T_) values were observed in the thalamus, striatum, and frontal cortex, with the lowest V_T_ value in the cerebellum. Kinetic modeling with the 2-tissue compartment model (2TCM) and Logan plot analysis provided better fits than 1TCM. The V_T_ values obtained with 2TCM correlated well with those from the Logan analysis (R^2^ = 0.957; P < 0.001). The Logan V_T_ values were 5, 6, 8, and 1 for the thalamus, striatum, frontal cortex, and cerebellum, respectively. No blocking or ex vivo biodistribution studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FE-PEO%20and%20human)]

No publication is currently available.

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
3 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
7 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
8 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
9 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
10 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
11 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
12 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
13 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
14 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
15 Lever J.R., Dannals R.F., Wilson A.A., Ravert H.T., Wagner H.N. (1987). Synthesis of carbon-11 labeled diprenorphine: a radioligand for positron emission tomographic studies of opiate receptors. Tetrahedron Letters.
16 Luthra S.K., Brady F., Turton D.R., Brown D.J., Dowsett K., Waters S.L., Jones A.K., Mathews R.W., Crowder J.C. (1994). Automated radiosyntheses of [6-O-methyl-11C]diprenorphine and [6-O-methyl-11C]buprenorphine from 3-O-trityl protected precursors. Appl Radiat Isot.
17 Melichar J.K., Hume S.P., Williams T.M., Daglish M.R., Taylor L.G., Ahmad R., Malizia A.L., Brooks D.J., Myles J.S., Lingford-Hughes A., Nutt D.J. (2005). Using [11C]diprenorphine to image opioid receptor occupancy by methadone in opioid addiction: clinical and preclinical studies. J Pharmacol Exp Ther.
18 Hume S.P., Lingford-Hughes A.R., Nataf V., Hirani E., Ahmad R., Davies A.N., Nutt D.J. (2007). Low sensitivity of the positron emission tomography ligand [11C]diprenorphine to agonist opiates. J Pharmacol Exp Ther.
19 Marton J., Schoultz B.W., Hjornevik T., Drzezga A., Yousefi B.H., Wester H.J., Willoch F., Henriksen G. (2009). Synthesis and evaluation of a full-agonist orvinol for PET-imaging of opioid receptors: [11C]PEO. J Med Chem.
20 Riss P.J., Hong Y.T., Marton J., Caprioli D., Williamson D.J., Ferrari V., Saigal N., Roth B.L., Henriksen G., Fryer T.D., Dalley J.W., Aigbirhio F.I. (2013). Synthesis and Evaluation of 18F-FE-PEO in Rodents: An 18F-Labeled Full Agonist for Opioid Receptor Imaging. J Nucl Med.